# [(Biotin-Ala-Ser-Lys-Lys-Pro-Lys-Arg-Asn-Ile-Lys-Ala)_4_-dendrimer]-streptavidin-[biotin-gadolinium 1,4,7-tris(carboxymethyl)-10-(2’-hydroxypropyl)-1,4,7,10-tetraazacyclododecane-loaded apoferritin]

Chemical name: | [(Biotin-Ala-Ser-Lys-Lys-Pro-Lys-Arg-Asn-Ile-Lys-Ala)_4_-dendrimer]-streptavidin-[biotin-gadolinium 1,4,7-tris(carboxymethyl)-10-(2’-hydroxypropyl)-1,4,7,10-tetraazacyclododecane-loaded apoferritin]
Abbreviated name: | C3d-SA-GdAF
Synonym:
Agent category: | Cage molecule
Target: | Neural cell adhesion molecule (NCAM)
Target cateogry: | Adhesion molecule
Method of detection: | Magnetic Resonance Imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadolinium apoferritin))]

The neural cell adhesion molecule (NCAM) is a cell surface glycoprotein that belongs to the immunoglobulin (Ig) super-family of cell adhesion molecules (CAMs) (1). One of its critical functions in embryogenesis, neural plasticity, tumor progression, and oncogenesis is to mediate cell–cell adhesion through homophilic NCAM binding (2). The extracellular part of NCAM consists of five Ig homology modules and two fibronectin type III (F3) modules (3). Evidence demonstrates that the homophilic interaction is mediated by a double reciprocal interaction between the IgI and IgII modules of two NCAM molecules (3). This homophilic NCAM–NCAM binding originates from a stretch of ~10 amino acids in the modules with a dissociation constant (K_d_) of 55 μM (1, 4). Many short peptides have been synthesized to explore the mechanism of this homophilic binding. For instance, C3 peptide, which contains a sequence of 11 amino acids (Ala-Ser-Lys-Lys-Pro-Lys-Arg-Asn-Ile-Lys-Ala (ASKKPKRNIKA)), is an NCAM IgI ligand selected from a combinatorial library of synthetic peptides (4). C3d is a C3 peptide dendrimer formed by coupling four C3 peptides to a lysine dendrimer. As a multimeric ligand, C3d has an increased potency for binding to the NCAM IgI module (K_d_ ~10 μM) compared to the monomer C3 peptide (4, 5). C3d can effectively disrupt NCAM-mediated cell adhesion, trigger intracellular signal cascades in vitro, and significantly modulate synaptic function in vivo (5).

[(Biotin-Ala-Ser-Lys-Lys-Pro-Lys-Arg-Asn-Ile-Lys-Ala)_4_-dendrimer]-streptavidin-[biotin-gadolinium 1,4,7-tris(carboxymethyl)-10-(2’-hydroxypropyl)-1,4,7,10-tetraazacyclododecane-loaded apoferritin] (C3d-SA-GdAF) is a magnetic resonance imaging (MRI) contrast agent used to image NCAM in vivo (6). C3d-SA-GdAF consists of three components, a biotinylated Gd-loaded apoferritin, a streptavidin, and a biotinylated C3d dendrimer (C3d-Bio). Streptavidin is tetrameric protein (molecular mass, 53 kDa) secreted from streptomyces bacteria and can provide four tightly noncovalent binding sites to biotin (molecular mass, 244 Da) with an extraordinarily high binding affinity (K_d_ ≈ 10^-15^–10^-16^ M) (7). The bond formed between streptavidin and biotin is a rapid, irreversible process that is unaffected by most extremes of pH, organic solvents, and denaturing reagents (8). Because only the bicyclic ring of biotin is recognized by the streptavidin, the carboxyl group in the biotin side chain is modified chemically to obtain reactive biotinyl derivatives (9). Proteins are generally biotinylated via amino groups by using an N-hydroxysuccinimide ester (NHS-ester) of a biotin analog. The steric hindrance between the biotin and the protein is normally reduced by adding an extra spacer arm, as found in the biotinyl agent NHS-LC-biotin (10). In C3d-SA-GdAF, both the peptide C3d (as a ligand of NCAM) and the Gd-loaded apoferritin (as a MRI contrast enhancer) are biotinylated. Streptavidin serves as a linker between the two biotinylated molecules to generate a NCAM-specific MRI contrast agent (6).

The Gd-loaded apoferritin is obtained by the entrapment of small Gd chelates inside an apoferritin molecule (11). Gd-1,4,7-Tris(carboxymethyl)-10-2(2’-hydroxypropyl)-1,4,7,10-tetraazacyclododecane (HPDO3A) is a neutral, highly hydrophilic contrast agent for clinical MRI. The coordination cage of Gd-HPDO3A is very tight (log k_f_ = 23.8) over a fairly large pH range and contains one structural water (q = 1) (11, 12). Apoferritin is a spherical protein with a shell of 12.5 nm and an empty central cavity of 7–8 nm (13). There are 14 channels 3–4 Å in diameter that are formed at the intersections of 24 subunits. These channels connect the outside of the apoferritin with its interior and allow the external molecules to access the inner cavity (13). Molecules such as water or that have a diameter <7 Å can diffuse through the channels but not the Gd-HPDO3A chelates (11). Because apoferritin can be dissociated into subunits at low pH (2.0) and the subunits can be reconstituted back to the apoferritin at a high pH (8.5), Gd-HPDO3As are trapped in the apoferritin cavity via this dissociation/reconstitution process (11, 13). Once trapped in the apoferritin cavity, Gd-HPDO3A exhibits a 20-fold increase in T_1_ relaxivity compared to the untrapped Gd-HPDO3A (11). This is the highest relaxivity reported thus far, and it has been attributed to the reduction in the effective rotational correlation time of the chelates and the strong dipolar interactions with the exchangeable protons on the protein surface in the proximity of paramagnetic chelates (11). The inner cavity of apoferritin possesses a large surface that can provide amplified dipolar interactions. In addition, as an endogenous protein, apoferritin causes no immune response and provides high stability for easy biotinylation of surface amino groups (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadolinium apoferritin)+AND+synthesis%0D%0A)]

C3d-SA-GdAF was obtained by mixing biotinylated Gd-loaded apoferritin, streptavidin, and biotinylated peptide dendrimer C3d (6). Aime et al. described the details of preparing Gd-loaded apoferritin (11). Apoferritin at a concentration of 0.01 mM was dissociated into 24 subunits by lowering the pH to 2 and maintaining for 15 min. Then 0.1 M Gd-HPDO3A was added to the protein solution and the pH was adjusted to 7.4. The resulting solution was stirred at room temperature for ~2 h to allow for sufficient entrapment of Gd chelates. Then the solution was dialyzed to remove the untrapped Gd-HPDO3A. Crich et al. reported the details of the biotinylation step (6). The biotinylation of Gd-loaded apoferritin was accomplished with the use of [N-(+)-biotinyl-6-aminocaproic acid N-succinimidyl ester (NHS-LC-biotin) according to standard protein modification protocols. Each apoferritin contained 5 ± 1 biotin residues as determined with the 2-(4’-hydroxyazobenzene) benzoic acid (HABA) colorimetric assay, as well as 8–10 molecules of Gd-HPDO3A as determined by inductively coupled plasma–mass spectrometer (ICP-MS). Crich et al. also detailed the synthesis of C3d-Bio (6). The peptide dendrimer C3d was obtained by standard Fmoc strategy with an Fmoc-Lys(Fmoc)-OH core and an Fmoc-PAL-PEG-PS resin. The biotinylation step was completed in solid phase using D-biotin and N,N,N',N'-tetramethyl-O-(7-azabenzotriazol-1-yl)uronium hexafluorophosphate (HTAU)/N,N-diisopropylethylamine (DIPEA). The final product, C3d-Bio, was obtained with 60% yield. Four biotin residues per C3d dendrimeric peptide were found with HABA colorimetric assay.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadolinium apoferritin)+AND+%22in+vitro%22)]

The in vitro binding experiments for C3d-Bio were tested in tumor-derived endothelial cells (TEC), which is a NCAM-positive cell line (2). The C3d-Bio demonstrated a dose-dependent binding specificity on the basis of cytofluorimetric analysis of phycoerythrin (PE)-conjugated streptavidin. The in vitro binding experiments for C3d-SA-GdAF were conducted in TEC again (6). C3d-Bio peptide, streptavidin, and Gd-loaded apoferritin were sequentially added to TEC at a molar ratio of 20:1:1 at 20°C, with a 20-min time interval between the addition of each component. The amount of Gd bound to cells was measured by ICP-MS. The T_1_ relaxivity was found to be ~70 ± 10 mM^-1^•s^-1^ at 0.47 T and 25°C. In comparison, the T_1_ relaxivity for Gd-HPDO3A was 3.7 ± 0.1 mM^-1^•s^-1^. The Gd-loaded apoferritin exhibited a relaxivity hump at ~35 MHz in its T_1_ nuclear magnetic resonance dispersion (NMRD) profile, demonstrating slow tumbling of the Gd chelates. For the Gd-loaded apoferritin-bound TEC, the T_1_ relaxivity appeared to have the same bell shape as the unbound apoferritin in the NMRD profile. MR images of the Gd-loaded apoferritin-bound TEC were acquired with a 7-T imager, which appeared to be hyperintense compared to control cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadolinium apoferritin) +AND++rodentia)]

The in vivo study was conducted in severe combined immunodeficient (SCID) mice with implanted TEC (6). First, 20 μmol/kg C3d-Bio was injected; 45 min later, 1 μmol/kg streptavidin and 1 μmol/kg Gd-loaded apoferritin were injected together. Each streptavidin molecule had three binding sites available for binding the biotin resides of C3d-Bio. Six days after implantation, T_1_-weighted images were collected with a 7-T imager before and 10.0 min, 5 h, 24 h, and 48 h after the contrast administration. Signal intensity (SI) enhancement was found to be ≥30% in the tumor after 5 h, and this decreased to 20% after 24 h. The SI enhancements in the liver, kidneys, and muscle were 85%, 30%, and 3%, respectively, after 5 h, indicating that the Gd complex remained inside the apoferritin cavity. The modified apoferritin was absorbed by the hepatocytes as the native protein and followed the protein elimination pathways through the liver uptake. In comparison, Gd-HPDO3A was excreted only through the kidneys. The in vivo binding of C3d-SA-GdAF at TEC-neoformed vessels was confirmed by immunofluorescence imaging after in vivo administration of fluorescein isothiocyanate (FITC)-labeled C3d-SA-GdAF.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadolinium apoferritin) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadolinium apoferritin) +AND+human)]

No publication is currently available.

## References

1 Kiselyov V.V., Soroka V., Berezin V., Bock E. (2005). Structural biology of NCAM homophilic binding and activation of FGFR. J Neurochem.
2 Bussolati B., Grange C., Bruno S., Buttiglieri S., Deregibus M.C., Tei L., Aime S., Camussi G. (2006). Neural-cell adhesion molecule (NCAM) expression by immature and tumor-derived endothelial cells favors cell organization into capillary-like structures. Exp Cell Res.
3 Ronn L.C., Olsen M., Soroka V. (2002). O.S. S, S. Dissing, F.M. Poulsen, A. Holm, V. Berezin, and E. Bock, Characterization of a novel NCAM ligand with a stimulatory effect on neurite outgrowth identified by screening a combinatorial peptide library. Eur J Neurosci.
4 Ronn L.C., Olsen M., Ostergaard S., Kiselyov V., Berezin V., Mortensen M.T., Lerche M.H., Jensen P.H., Soroka V., Saffell J.L., Doherty P., Poulsen F.M., Bock E., Holm A. (1999). Identification of a neuritogenic ligand of the neural cell adhesion molecule using a combinatorial library of synthetic peptides. Nat Biotechnol.
5 Kiryushko D., Kofoed T., Skladchikova G., Holm A., Berezin V., Bock E. (2003). A synthetic peptide ligand of neural cell adhesion molecule (NCAM), C3d, promotes neuritogenesis and synaptogenesis and modulates presynaptic function in primary cultures of rat hippocampal neurons. J Biol Chem.
6 Geninatti Crich S., Bussolati B., Tei L., Grange C., Esposito G., Lanzardo S., Camussi G., Aime S. (2006). Magnetic resonance visualization of tumor angiogenesis by targeting neural cell adhesion molecules with the highly sensitive gadolinium-loaded apoferritin probe. Cancer Res.
7 Laitinen O.H., Hytonen V.P., Nordlund H.R., Kulomaa M.S. (2006). Genetically engineered avidins and streptavidins. Cell Mol Life Sci.
8 Laitinen O.H., Nordlund H.R., Hytonen V.P., Kulomaa M.S. (2007). Brave new (strept)avidins in biotechnology. Trends Biotechnol.
9 Wilchek M., Bayer E.A. (1988). The avidin-biotin complex in bioanalytical applications. Anal Biochem.
10 Diamandis E.P., Christopoulos T.K. (1991). The biotin-(strept)avidin system: principles and applications in biotechnology. Clin Chem.
11 Aime S., Frullano L., Geninatti Crich S. (2002). Compartmentalization of a gadolinium complex in the apoferritin cavity: a route to obtain high relaxivity contrast agents for magnetic resonance imaging. Angew Chem Int Ed Engl.
12 Girard E., Chantalat L., Vicat J., Kahn R. (2002). Gd-HPDO3A, a complex to obtain high-phasing-power heavy-atom derivatives for SAD and MAD experiments: results with tetragonal hen egg-white lysozyme. Acta Crystallogr D Biol Crystallogr.
13 Webb B., Frame J., Zhao Z., Lee M.L., Watt G.D. (1994). Molecular entrapment of small molecules within the interior of horse spleen ferritin. Arch Biochem Biophys.